# ^17^O-Labeled water

Chemical name: | ^17^O-Labeled water
Abbreviated name: | H_2_^17^O
Synonym:
Agent category: | Compound
Target: | Blood flow
Target category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | ^17^O
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

The human brain (5% of total body weight) accounts for ~20% of total body oxygen consumption (2). Oxygen is consumed to produce water via oxidative phosphorylation and reoxidation of reduced molecules in the mitochondria. The cerebral rate of oxygen consumption (CMRO_2_) and the cerebral blood flow (CBF) are sensitive and quantitative indicators of the health of the brain. Reduced cerebral perfusion and oxygen consumption have been observed in neurodegenerative and cerebrovascular diseases. CMRO_2_ has been imaged using ^15^O positron emission tomography (PET) to monitor the H_2_^15^O concentration in the brain during inhalation of ^15^O_2_ (3, 4). However, ^15^O PET is not popular because of the short half-life (~2 min) of ^15^O, on-site generation of ^15^O_2_, and high background noise (^15^O_2_ bound to hemoglobin versus H_2_^15^O). CMRO_2_ has also been measured with ^17^O nuclear magnetic resonance (NMR) spectroscopy and MRI after inhalation of ^17^O_2_, which is converted to H_2_^17^O (5, 6). ^17^O cannot be detected because molecular ^17^O_2_ is dissolved in the blood or is bound to hemoglobin as ^17^O_2_. ^17^O is detectable as in H_2_^17^O. ^17^O decreases the proton T2 relaxation time of water as the direct method of NMR/MRI measurement. The other method is indirect MRI measurement based on the enhancement of T1p relaxation of protons in water by ^17^O. CMRO_2_ and CBF can be measured with ^17^O NMR spectroscopy and MRI after inhalation of ^17^O_2_. CBF can be measured with ^17^O NMR spectroscopy and MRI after injection of H_2_^17^O.

### Related Resource Links:

- Clinical trials (^15^O-water (http://www.clinicaltrials.gov/ct2/results?term=15O+water))
- ^15^O-water information in FDA (http://google2.fda.gov/search?q=15O-water&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=14)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI%20+and+synthesis)]

^17^O_2_ and H_2_^17^O are available commercially. No details of their synthesis were reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI+and+in+vitro)]

Zhu et al. (6) performed NMR measurement of T1 and T2 relaxation times of H_2_^17^O in saline solution at 4.7 T. The T1 and T2 values were 6.59 and 4.28 ms, respectively. The T1 and T2 values at 9.4 T were similar to those at 4.7 T.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI+and+rodentia)]

Tailor et al. (7) performed ^1^H T1p-weighted MRI of RIF-1 tumors in rats at 4 T to measure tumor blood flow (TBF) after intravenous injection of H_2_^17^O. Tumor heterogeneity with respect to TBF was clearly visible. The TBF was estimated to be 0.03 ml/g/min.

In another study, Tailor et al. (8) delivered H_2_^17^O to the rat brain via the right common carotid artery. ^1^H T1p-weighted MRI of the brain was performed at 4 T. The CBF values (n = 3) for the upper parieto-occipital cortex, lower parieto-occipital cortex, and combined thalamic and rostal mesencephalic region were 0.42 ± 0.09 ml/g/min, 0.49 ± 0.06 ml/g/min, and 0.89 ± 0.27 ml/g/min, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI+and+(dog+or+sheep+or+pig+or+rabbit))]

Arai et al. (9) measured CBF in cats with MRI using H_2_^17^O. The CBF values for the gray and white matter were 0.69 ± 0.10 ml/g/min (n = 8) and 0.37 ± 0.05 ml/g/min (n = 4), respectively. In hypercapnia, the CBF values for the gray and white matter increased to 1.59 ± 0.43 ml/g/min (n = 8) and 0.81 ± 0.18 ml/g/min (n = 4), respectively.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Oxygen-17%20MRI+and+human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Shulman R.G., Rothman D.L., Behar K.L., Hyder F. (2004). Energetic basis of brain activity: implications for neuroimaging. Trends Neurosci.
3 Leenders K.L., Perani D., Lammertsma A.A., Heather J.D., Buckingham P., Healy M.J., Gibbs J.M., Wise R.J., Hatazawa J., Herold S., et al. (1990). Cerebral blood flow, blood volume and oxygen utilization. Normal values and effect of age. Brain.
4 Mintun M.A., Raichle M.E., Martin W.R., Herscovitch P. (1984). Brain oxygen utilization measured with O-15 radiotracers and positron emission tomography. J Nucl Med.
5 Tailor D.R., Baumgardner J.E., Regatte R.R., Leigh J.S., Reddy R. (2004). Proton MRI of metabolically produced H2 17O using an efficient 17O2 delivery system. Neuroimage.
6 Zhu X.H., Merkle H., Kwag J.H., Ugurbil K., Chen W. (2001). 17O relaxation time and NMR sensitivity of cerebral water and their field dependence. Magn Reson Med.
7 Tailor D.R., Poptani H., Glickson J.D., Leigh J.S., Reddy R. (2003). High-resolution assessment of blood flow in murine RIF-1 tumors by monitoring uptake of H(2)(17)O with proton T(1rho)-weighted imaging. Magn Reson Med.
8 Tailor D.R., Roy A., Regatte R.R., Charagundla S.R., McLaughlin A.C., Leigh J.S., Reddy R. (2003). Indirect 17(O)-magnetic resonance imaging of cerebral blood flow in the rat. Magn Reson Med.
9 Arai T., Nakao S., Morikawa S., Inubushi T., Yokoi T., Shimizu K., Mori K. (1998). Measurement of local cerebral blood flow by magnetic resonance imaging: in vivo autoradiographic strategy using 17O-labeled water. Brain Res Bull.